# [^18^F]Fluorobenzyl-PEG_3_-Glu-c(RGDyK)-bombesin[7-14]

Chemical name: | [^18^F]Fluorobenzyl-PEG_3_-Glu-c(RGDyK)-bombesin[7-14]
Abbreviated name: | [^18^F]FB-PEG_3_-Glu-RGD-BBN
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR), integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids), which binds to GRP receptors (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system and the gastrointestinal system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-R) have been identified on central nervous system and gastrointestinal tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B (NMB) receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (7). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (8-13). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (12, 14, 15). A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various ligands have been introduced for imaging of tumors and tumor angiogenesis (16).

Because prostate cancer expresses both GRPR and α_v_β_3_, Liu et al. (17) designed an RGD-BBN heterodimer in which BBN[7-14] and c(RGDyK) were connected with a glutamate linker (BBN on the Glu side-chain γ-carboxylate group and on the Glu side-chain α-carboxylate group). A spacer, 11-amino-3,6,9-trioxaundecanoic acid (PEG_3_), was placed on the glutamate α-amino group of Glu-RGD-BBN to increase the hydrophilicity and to relieve the steric hindrance. N-Succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB) was used to synthesize [^18^F]FB-PEG_3_-Glu-RGD-BBN for tumor imaging in vivo.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+synthesis)]

Glu-RGD-BBN was prepared with solid-phase peptide synthesis with subsequent addition of a PEG_3_ group to form PEG_3_-Glu-RGD-BBN (17). [^18^F]SFB was added to a solution of PEG_3_-Glu-RGD-BBN. The mixture was heated for 30 min at 60°C. The product, [^18^F]FB-PEG_3_-Glu-RGD-BBN, was purified with high-performance liquid chromatography with a yield of 42% based on [^18^F]SFB and a radiochemical purity of >99%. The specific activity of [^18^F]FB-PEG_3_-Glu-RGD-BBN was estimated to be ~100 GBq/µmol (2.7 Ci/µmol) at the end of synthesis. [^18^F]FB is conjugated to the amino group of PEG_3_.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+in+vitro)]

Liu et al. (17) performed in vitro inhibition studies of RGD, PEG_3_-Glu-RGD-BBN, and FB-PEG_3_-Glu-RGD-BBN in cultured U87MG cells with ^125^I-echistatin. The 50% inhibition concentration (IC_50_) values were 11.2, 10.8, and 13.8 nM, respectively. In vitro inhibition studies of Aca-BBN, PEG_3_-Glu-RGD-BBN, and FB-PEG_3_-Glu-RGD-BBN were also performed in cultured PC-3 cells with ^125^I-BBN. The IC_50_ values were 79.0, 85.5, and 73.3 nM, respectively. Therefore, the FB-PEG_3_-RGD-BBN heterodimer exhibited comparable binding affinities for α_v_β_3_ integrin with GRPR and α_v_β_3_ integrin receptor as the parent RGD and BNN peptides. PC-3 cells express a high level of GRPR and a moderate level of α_v_β_3_ integrin. PC-3 cells exhibited a 5.9% and 2.5% uptake of incubation doses of [^18^F]FB-PEG_3_-Glu-RGD-BBN within 60 min of incubation at 37°C and4°C , respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+%20rodentia)]

Positron emission tomography (PET) scans were performed after intravenous injection of 3.7 MBq (100 μCi) [^18^F]FB-PEG_3_-Glu-RGD-BBN in nude mice (n = 4) bearing PC-3 tumors at 30, 60, and 120 min (17). The estimated accumulation of [^18^F]FB-PEG_3_-Glu-RGD-BBN in the PC-3 tumors was 6.4 ± 2.5% injected dose per gram (ID/g) at 30 min; radioactivity decreased to 4.4 ± 0.7% ID/g at 1 h and 2.5 ± 0.8% ID/g at 2 h after injection. The organs with the highest radioactivity were the kidney (~4% ID/g at 60 min) and liver (<1% ID/g at 60 min). The tumor/blood, tumor/liver, tumor/kidney, and tumor/muscle ratios were 8.10, 6.43, 1.44, and 10.54, respectively. [^18^F]FB-PEG_3_-Glu-RGD-BBN exhibited higher tumor/organ ratios than [^18^F]FB-Glu-BBN-RGD. BBN, c(RGDyK), or BBN+c(RGDyK) were co-injected with [^18^F]FB-PEG_3_-Glu-RGD-BBN in mice bearing PC-3 tumors. Tumor accumulation at 1 h after injection (4.4% ID/g) was only partially inhibited by either BBN (65% inhibition) or RGD (50% inhibition) alone. However, BBN+RGD reduced the tumor accumulation to the background level (90% inhibition). Ex vivo biodistribution at 1 h after injection confirmed the PET imaging biodistribution analysis in the kidney, tumor, liver, and muscle but also showed high accumulation (2–4% ID/g) in the pancreas, intestine, stomach, and spleen, which possess high GRPR levels. Accumulated radioactivity in the bone was low (<0.5% ID/g).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+human)]

No publication is currently available.

## NIH Support

R01 CA120188, R01 CA119053, R21 CA121842, R21 CA102123, P50 CA114747, U54 CA119367, R24 CA93862

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Smith C.J., Volkert W.A., Hoffman T.J. (2005). Radiolabeled peptide conjugates for targeting of the bombesin receptor superfamily subtypes. Nucl Med Biol.
7 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
8 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
9 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
10 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
11 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
12 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
13 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
14 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
15 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
16 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
17 Liu Z., Yan Y., Chin F.T., Wang F., Chen X. (2009). Dual integrin and gastrin-releasing peptide receptor targeted tumor imaging using 18F-labeled PEGylated RGD-bombesin heterodimer 18F-FB-PEG3-Glu-RGD-BBN. J Med Chem.